# IRDye 800CW-Anti-epidermal growth factor receptor nanobody 7D12

Chemical name: | IRDye 800CW-Anti-epidermal growth factor receptor nanobody 7D12
Abbreviated name: | IRDye800CW-7D12, IRDye800-7D12, 7D12-IR
Synonym:
Agent category: | Antibody fragment, nanobody
Target: | Epidermal growth factor receptor (EGFR, HER1)
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | IRDye 800CW
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4503491), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001963.2) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=1950) for more information about EGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20)]

Epidermal growth factor (EGF) is a 53-amino acid growth factor (6.2 kDa) that is secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF and at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2; however, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non–small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis because high levels are related to increased proliferation (7-10).

Trastuzumab, a humanized immunoglobulin G_1_ (IgG_1_) monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 (11), was labeled as ^111^In-trastuzumab (http://www.ncbi.nlm.nih.gov/books/NBK23144/) (12-14). C225, an anti-EGFR (HER1), mouse-human chimeric, monoclonal IgG_1_ antibody, also known as erbitux or cetuximab, was labeled as ^99m^Tc-EC-C225 (http://www.ncbi.nlm.nih.gov/books/NBK23305/) (15, 16) for imaging EGFR expression on solid tumors using single-photon emission computed tomography (SPECT). However, the pharmacokinetics of the intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging (17, 18). Smaller antibody fragments, such as scFv, Fab, or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. Nanobodies are the smallest intact antigen-binding fragments (15 kDa) isolated from heavy-chain camelid antibodies and exhibit efficient and specific tumor targeting (19-21). Nanobody 7D12 was labeled with ^99m^Tc at its C-terminus hexahistidine tail for SPECT (22) and with ^68^Ga and ^89^Zr for positron emission tomography (PET) (23) imaging EGFR (HER1) expression in tumors in mice. Oliveira et al. (24) prepared IRDye 800CW-anti-EGFR nanobody 7D12 for near-infrared (NIR) fluorescence imaging studies in tumor-bearing mice. IRDye 800CW is an indocyanine-type NIR fluorophore with peak absorption at 785 nm and peak excitation emission at 803 nm. Fluorescence imaging has an advantage in sensitivity in small animals where the signal is not degraded by significant absorption.

### Related Resource Links:

- Chapters in MICAD (EGFR (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad), 7D12 (http://www.ncbi.nlm.nih.gov/books?term=7d12%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (EGFR (http://www.ncbi.nlm.nih.gov/gene/1956))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EGFR (http://www.ncbi.nlm.nih.gov/omim/131550))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab), cetuximab (http://www.clinicaltrials.gov/ct2/results?term=Cetuximab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14), cetuximab (http://google2.fda.gov/search?q=Cetuximab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=7&y=18))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20and%20synthesis)]

Commercially available IRDye 800CW-N-hydroxysuccinimide ester (LI-COR, Lincoln, NE) was used to conjugate 7D12 to form IRDye800CW-7D12, which was purified with gel filtration chromatography to a purity of >92% (24). The molar ratio of IRDye 800CW to 7D12 was estimated to be 0.5 with gel permeation chromatography. It has a molecular weight of ~16 kDa based on gel electrophoresis analysis. IRDye800CW-Cetuximab and control nanobody IRDye800CW-R2 were also prepared with 1.4 and 1.1 dye/protein ratios, respectively. IRDye800CW-Conjugated proteins were >98% intact in phosphate-buffered saline at 4°C for up to 100 days and in serum at 37°C for up to 7 days.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20and%20in%20vitro)]

Binding experiments were performed with the nanobody 7D12 alone with the use of a Biacore sensor chip immobilized with extracellular domain of EGFR protein (22). The K_d_ value of 7D12 was calculated to be 5.7 nM.

Saturation binding studies were performed with EGFR-expressing 14C cells at 4°C (24). The K_d_ values were 0.5, 0.05, 2, 1, and >10,000 nM for IRDye800CW-cetuximab, cetuximab, IRDye800CW-7D12, 7D12, and IRDye800CW-R2, respectively. Dye conjugations had little effect on the binding affinities of IRDye800CW-7D12 and 7D12, whereas there was a larger difference between IRDye800CW-cetuximab and cetuximab.

Three murine fibroblasts (NIH 3T3, 3T3 2.2, HER14) and three human tumor cell lines expressing different levels of EGFR (A431 > 14C > HeLa) were incubated with 12.5 nmol IRDye800CW-7D12, IRDye800CW-cetuximab, and IRDye800CW-R2 for 2 h at 4°C (24). The extent of binding of IRDye800CW-7D12 and IRDye800CW-cetuximab was correlated with the amount of EGFR expression in these cell lines. The binding of IRDye800CW-7D12 (25 nM) to 14C cells was inhibited by 40%, 80%, and 95% with 25, 250, and 2,500 nM EGF, respectively. The binding of IRDye800CW-7D12 and IRDye800CW-cetuximab to 14C cells was inhibited by 95% and 85% with excess cetuximab, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20and%20rodentia)]

Oliveira et al. (24) performed ex vivo biodistribution studies of IRDye800CW-7D12 (1.6 nmol/mouse), IRDye800CW-cetuximab (0.67 nmol/mouse), and IRDye800CW-R2 (1.6 nmol/mouse) in A431 tumor-bearing nude mice (n = 5/group) at 2 h and 24 h after injection. Accumulation of IRDye800CW-7D12 into A431 tumors was 17% injected dose/gram (ID/g) at 2 h and decreased to 8% ID/g at 24 h. On the other hand, accumulation of IRDye800CW-cetuximab into A431 tumors was 5% ID/g at 2 h and increased to 8% ID/g at 24 h. Minimal accumulation of IRDye800CW-R2 in tumors was observed at 2 h and 24 h. IRDye800CW-7D12 and IRDye800CW-R2 exhibited high kidney accumulation, whereas IRDye800CW-cetuximab exhibited high liver accumulation. The tumor/normal organ ratios for IRDye800CW-7D12 were higher than those for IRDye800CW-cetuximab and IRDye800CW-R2 at 2 h and 24 h. Pretreatment of mice with 6.7 nmol cetuximab 48 h before injection of IRDye800CW-7D12 or IRDye800CW-cetuximab showed that there was ~70% reduction of IRDye800CW-cetuximab fluorescence in the tumors at 24 h after injection, whereas only ~30% reduction of IRDye800CW-7D12 fluorescence was observed in the tumors at 2 h after injection. The investigators suggested that the reduced blocking with cetuximab may be due to less effective penetration of cetuximab into the tumors to block the accumulation of IRDye800CW-7D12. No blocking studies were performed with unlabeled 7D12. Fluorescence microscopy of tumor sections revealed that the NIR fluorescence of IRDye800CW-7D12 was homogeneously distributed throughout the tumors and in the core of the tumors at 2 h after injection, whereas the NIR fluorescence intensities of IRDye800CW-cetuximab and IRDye800CW-R2 were distributed mainly in the periphery of the tumors at 24 h and 2 h after injection, respectively.

A whole-body NIR fluorescence imaging study was performed in A431 tumor-bearing nude mice (n = 4/group) at 0.25, 0.5, 1, 2, 3, 4, 5, 6, 24, 48, and 72 h after injection of IRDye800CW-7D12, IRDye800CW-cetuximab, and IRDye800CW-R2 (24). The tumors were clearly visualized at 30 min after injection of IRDye800CW-7D12, whereas minimal fluorescence was detected at 30 min after injection of IRDye800CW-cetuximab. The highest contrast of the tumors with IRDye800CW-7D12 and IRDye800CW-cetuximab was at 2 h and 24 h after injection, respectively. The small size of IRDye800CW-7D12 (~16 kDa) was able to penetrate the leaky tumor vasculatures faster than the large size of IRDye800CW-cetuximab (~150 kDa). Minimal fluorescence with IRDye800CW-R2 was detected at these time points. No blocking studies were performed with unlabeled 7D12.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=7D12%20nanobody%20and%20human)]

No publication is currently available.

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer: signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Schechter N.R., Yang D.J., Azhdarinia A., Kohanim S., Wendt R., Oh C.S., Hu M., Yu D.F., Bryant J., Ang K.K., Forster K.M., Kim E.E., Podoloff D.A. (2003). Assessment of epidermal growth factor receptor with 99mTc-ethylenedicysteine-C225 monoclonal antibody. Anticancer Drugs.
16 Schechter N.R., Wendt R.E., Yang D.J., Azhdarinia A., Erwin W.D., Stachowiak A.M., Broemeling L.D., Kim E.E., Cox J.D., Podoloff D.A., Ang K.K. (2004). Radiation dosimetry of 99mTc-labeled C225 in patients with squamous cell carcinoma of the head and neck. J Nucl Med.
17 Olafsen T., Wu A.M. (2010). Antibody vectors for imaging. Semin Nucl Med.
18 Wu A.M. (2009). Antibodies and antimatter: the resurgence of immuno-PET. J Nucl Med.
19 Arbabi Ghahroudi M., Desmyter A., Wyns L., Hamers R., Muyldermans S. (1997). Selection and identification of single domain antibody fragments from camel heavy-chain antibodies. FEBS Lett.
20 Desmyter A., Decanniere K., Muyldermans S., Wyns L. (2001). Antigen specificity and high affinity binding provided by one single loop of a camel single-domain antibody. J Biol Chem.
21 Muyldermans S. (2001). Single domain camel antibodies: current status. J Biotechnol.
22 Gainkam L.O., Huang L., Caveliers V., Keyaerts M., Hernot S., Vaneycken I., Vanhove C., Revets H., De Baetselier P., Lahoutte T. (2008). Comparison of the biodistribution and tumor targeting of two 99mTc-labeled anti-EGFR nanobodies in mice, using pinhole SPECT/micro-CT. J Nucl Med.
23 Vosjan M.J., Perk L.R., Roovers R.C., Visser G.W., Stigter-van Walsum M., van Bergen En Henegouwen P.M., van Dongen G.A. (2011). Facile labelling of an anti-epidermal growth factor receptor Nanobody with 68Ga via a novel bifunctional desferal chelate for immuno-PET. Eur J Nucl Med Mol Imaging.
24 Oliveira S., van Dongen G.A., Stigter-van Walsum M., Roovers R.C., Stam J.C., Mali W., van Diest P.J., van Bergen En Henegouwen P.M. (2012). Rapid Visualization of Human Tumor Xenografts through Optical Imaging with a Near-infrared Fluorescent Anti-Epidermal Growth Factor Receptor Nanobody. Mol Imaging.